# ^11^C-Labeled Telmisartan, an angiotensin II type 1 receptor antagonist

Chemical name: | ^11^C-Labeled Telmisartan, an angiotensin II type 1 receptor antagonist | [image]
Abbreviated name: | [^11^C]Telmisartan | [image]
Synonym: | | [image]
Agent Category: | Compound | [image]
Target: | Angiotensin II type 1 receptor | [image]
Target Category: | Receptor | [image]
Method of detection: | Positron emission tomography | [image]
Source of signal / contrast: | ^11^C | [image]
Activation: | No | [image]
Studies: | - Rodents; - Humans | Structure of [^11^C]Telmisartan.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Angiotensin%20II%20receptors&cmd=DetailsSearch)]

Angiotensin II (Ang II), a product of the renin-angiotensin system, mediates the activity of this system primarily through two receptors: the Ang II type 1 receptor (AT_1_R) and the Ang II type 2 receptor (AT_2_R) (1). Both of these receptors (ATRs) are known to play an important role in the regulation of arterial blood pressure and to participate in the development of heart failure, ischemic heart disease, renal failure, and various cerebrovascular pathologies in humans (2). The signal transduction and interaction of the AT_1_R and AT_2_R, and their modulation of the cardiovascular system, are discussed in detail elsewhere (1, 2). Because the AT_1_R regulates blood pressure, drugs such as telmisartan (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=cfb9309f-e0df-4a55-9542-0e869fce05fb#nlm34089-3), a non-peptide selective antagonist of AT_1_R, are often used to treat clinical hypertension and to reduce cardiovascular risk in patients. Studies have shown that telmisartan is converted into its glucuronide derivative in the liver for inactivation and excretion through the hepatobiliary system (3, 4). Investigations have shown that this drug exhibits an inconsistent and nonlinear plasma pharmacokinetic profile when increasing doses of the drug are given to rodents and humans (3, 4). The organic anion-transporting polypeptide 1B3 (OATP1B3) that is expressed on the sinusoidal membrane of the hepatocytes is known to transport telmisartan and other drugs into these cells (5). Therefore, OATP1B3 controls the clearance of telmisartan from the liver, and saturation of the OATP1B3-assisted uptake at high doses is believed to cause the nonlinear pharmacokinetics observed in humans who are administered telmisartan (4). However, it is not feasible to measure the in vivo transport of a drug from blood circulation into the liver because it is difficult to determine the drug concentrations accurately in animal or human hepatic tissue (3, 4).

Takashima et al. showed that positron emission tomography (PET) imaging can be used to investigate the quantitative hepatobiliary transport of the methyl ester of (15R)-16-m-[^11^C]tolyl-17,18,19,20-tetranorisocarbacyclin by the multidrug resistance-associated protein 2 transporter (6). On the basis of these observations, ^11^C-labeled telmisartan was synthesized (7) and used to study the biodistribution, pharmacokinetics, and transport function of OATP1B3 with PET imaging in rats (3) and humans (4). This chapter presents only the biodistribution and PET imaging results obtained with [^11^C]telmisartan (3, 4).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Angiotensin+receptor+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://www.clinicaltrials.gov/ct2/results?term=Angiotensin+II+receptor) related to angiotensin II receptor

Human angiotensin II receptor type 1 gene (http://www.ncbi.nlm.nih.gov/gene/185)

Angiotensin II receptor in Online Mendelian Inheritance in Man database (OMIM (http://omim.org/entry/106165))

Renin-angiotensin system pathways in humans (http://www.genome.jp/kegg-bin/show_pathway?hsa04614)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5DTelmisartan%20synthesis&cmd=DetailsSearch)]

The automated synthesis of [^11^C]telmisartan has been described by Iimori et al. (7). The purified tracer was formulated in 0.9% sodium chloride containing 0.03% ethanol and 0.05% polyethylene-glycol 400 (concentration not reported) and passed through a 0.22-μm filter into a pyrogen-free vial for storage (conditions not mentioned) until required. The radiochemical yield of [^11^C]telmisartan was 16.8 ± 2.9% at the end of bombardment (n = 8 reactions), and the time taken to complete the synthesis was 32–36 min. The radiochemical purity of the final product was >97%, with a specific activity of >86.3 MBq/nmol (3.193 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5DTelmisartan%20in%20vitro&cmd=DetailsSearch)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5DTelmisartan%20rodentia&cmd=DetailsSearch)]

The tissue distribution (in blood, liver, and intestines) and the hepatobiliary transport of [^11^C]telmisartan were investigated in rats as described by Takashima et al. (3). The anesthetized animals (n = 3 rats/set of experiments) were administered a bolus injection of the tracer (57–134 MBq/kg (2.1–4.9 mCi/kg) body weight (BW); 0.2–1.4 nmol/body) through the tail vein either alone (controls), after an infusion of 0.5 or 1.5 μmol/min per kg BW rifampicin (a functional inhibitor of OATP given at least 90 min before the administration of [^11^C]telmisartan; the infusion was continued up to the end of the study), or as a mixture with increasing doses of nonradioactive telmisartan (1.9, 7.6, and 19.4 μmol/min per kg BW, respectively). In control rats, 55 ± 1% of the injected dose (% ID) of the radiochemical was detected in the liver at 14 min postinjection (p.i.), and the accumulation of radioactivity in this organ gradually decreased thereafter for up to 90 min p.i. During the same period, the amount of tracer increased in the intestine (this corresponds to the amount of radioactivity in the bile that is excreted into the intestine) from ~5% ID at ~2.5 min p.i. to 20 ± 4% ID at 90 min p.i. The amount of tracer in the blood decreased from ~10% ID at ~1 min p.i. to ~0.5% at 90 min p.i. The uptake of [^11^C]telmisartan-associated radioactivity in blood, liver, and intestine of rats infused with the different doses of rifampicin is presented in Table 1. Animals infused with rifampicin showed a dose-dependent decrease in the uptake of label in the liver and the intestines compared with controls (3). In addition, the amount of label in the blood was 2.4-fold and 3.9-fold higher in rats infused with 0.5 and 1.5 μmol/min per kg BW rifampicin, respectively. These results indicated that the tracer from [^11^C]telmisartan was excreted primarily through the hepatobiliary system in the rodents.

Table 1: Uptake of radioactivity from [ ^ 11 ^ C]telmisartan in blood, liver, and intestine of rats infused with different doses of rifampicin ( 3 ).

Tissue/Organ | Control | | Rifampicin Dose (μmol/min per kg body weight )
Tissue/Organ | Control | | 0.5 | | 1.5
Tissue/Organ | Time (min) postinjection
Tissue/Organ | 1 | 90 | 1 | 90 | 1 | 90
Tissue/Organ | Radioactivity (% ID)
Blood | 8 | 0.08 | 8 | 0.2 | 8 | 0.4
Liver | 48 | 45 | 45 | 40 | 40 | 30
Intestine | 5 | 18 | 4 | 10 | 4 | 10

Data presented in this Table are approximate.

The amount of radioactivity from [^11^C]telmisartan present in the blood, liver, and intestine of rats pretreated with increasing concentration of nonradioactive telmisartan is presented in Table 2.

Table 2: Accumulated radioactivity from [ ^ 11 ^ C]telmisartan in blood, liver, and intestine of rats pretreated with nonradioactive telmisartan ( 3 ).

Tissue/Organ | Control | | Nonradioactive Telmisartan Dose (μmol/kg body weight)
Tissue/Organ | Control | | 2 | | 4 | | 20
Tissue/Organ | Time (min) postinjection
Tissue/Organ | 1 | 90 | 1 | 90 | 1 | 90 | 1 | 90
Tissue/Organ | Radioactivity (% ID)
Blood | 8 | 0.08 | 8 | 0.09 | 8 | 0.11 | 8 | 0.11
Liver | 50 | 46 | 50 | 44 | 38 | 32 | 30 | 25
Intestine | 4 | 18 | 4 | 18 | 6 | 32 | 8 | 40

Data presented in this Table are approximate.

A low dose of nonradioactive telmisartan (2 μmol/kg BW) did not change the amount of label from [^11^C]telmisartan in the blood, liver, and intestine of the rats (3). At higher doses (4 and 20 μmol/kg BW), the amount of radioactivity in the liver decreased from 1 min to 90 min p.i., but the amount of label in the blood and the intestine was observed to increase during the same period.

PET imaging of control rats and animals pretreated with rifampicin or nonradioactive telmisartan revealed that the radioactivity was localized primarily in the liver at 2 min p.i., and subsequently a part of the radioactivity moved into the intestine (3). The amount of radioactivity detected in the intestine corresponded to the amount of label excreted into the bile.

In another study with rats (n = 3 animals), radioactivity from [^11^C]telmisartan was shown to be taken up rapidly by the liver, and a part of it was excreted into the bile ducts and the intestine of the rodents (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5DTelmisartan%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5DTelmisartan%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5DTelmisartan%20Human%20Studies&cmd=DetailsSearch)]

The biodistribution of [^11^C]telmisartan was investigated in healthy human volunteers (n = 6 individuals; average weight, 58.5 ± 2.8 kg) as described by Shimizu et al. (4). Each subject was given an intravenous bolus injection of 106 ± 8.7 MBq (3.9 ± 0.32 mCi) [^11^C]telmisartan (specific activity, 54.5 ± 13.8 MBq/nmol (2.01 ± 0.51 mCi/nmol), and dynamic whole-body PET images were acquired from the individuals for up to 120 min p.i. PET scans acquired immediately after the administration of [^11^C]telmisartan showed that the radioactivity accumulated primarily in the liver and was gradually excreted into the gall bladder and then into the intestine of all the individuals. During the early phase of the study, the other organs (kidneys, intestine, and the urinary bladder) were not visible clearly. Maximum uptake of [^11^C]telmisartan was observed in the liver (55.7 ± 3.3% ID at 0.80 h p.i.). The peak amounts of tracer observed in the brain, lungs, heart, and kidneys were 1.6 ± 0.5% ID, 2.8 ± 0.7% ID, 3.1 ± 0.4% ID, and 3.7 ± 0.3% ID, respectively, at 4.5 min p.i. The maximum amount of label in the gall bladder and small intestine was 5.3 ± 6.6% ID and 8.7 ± 2.8% ID, respectively, at 81 min p.i.

From this study, the investigators concluded that [^11^C]telmisartan was a safe PET agent for use in humans (4).

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Horiuchi M., Iwanami J., Mogi M. (2012). Regulation of angiotensin II receptors beyond the classical pathway. Clin Sci (Lond).
2 Savoia C., Volpe M. (2011). Angiotensin receptor modulation and cardiovascular remodeling. J Renin Angiotensin Aldosterone Syst.
3 Takashima T., Hashizume Y., Katayama Y., Murai M., Wada Y., Maeda K., Sugiyama Y., Watanabe Y. (2011). The involvement of organic anion transporting polypeptide in the hepatic uptake of telmisartan in rats: PET studies with [(1)(1)C]telmisartan. Mol Pharm.
4 Shimizu K., Takashima T., Yamane T., Sasaki M., Kageyama H., Hashizume Y., Maeda K., Sugiyama Y., Watanabe Y., Senda M. (2012). Whole-body distribution and radiation dosimetry of [(11)C]telmisartan as a biomarker for hepatic organic anion transporting polypeptide (OATP) 1B3. Nucl Med Biol.
5 Ishiguro N., Maeda K., Kishimoto W., Saito A., Harada A., Ebner T., Roth W., Igarashi T., Sugiyama Y. (2006). Predominant contribution of OATP1B3 to the hepatic uptake of telmisartan, an angiotensin II receptor antagonist, in humans. Drug Metab Dispos.
6 Takashima T., Nagata H., Nakae T., Cui Y., Wada Y., Kitamura S., Doi H., Suzuki M., Maeda K., Kusuhara H., Sugiyama Y., Watanabe Y. (2010). Positron emission tomography studies using (15R)-16-m-[11C]tolyl-17,18,19,20-tetranorisocarbacyclin methyl ester for the evaluation of hepatobiliary transport. J Pharmacol Exp Ther.
7 Iimori H., Hashizume Y., Sasaki M., Kajiwara Y., Sugimoto Y., Sugiyama Y., Watanabe Y., Senda M. (2011). First automatic radiosynthesis of 11C labeled Telmisartan using a multipurpose synthesizer for clinical research use. Ann Nucl Med.